# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-vascular endothelial growth factor-121(D63AE64AE67A)

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-vascular endothelial growth factor-121(D63AE64AE67A)
Abbreviated name: | ^64^Cu-DOTA-VEGF_DEE_
Synonym:
Agent Category: | Polypeptide
Target: | VEGF receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE))]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (1).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). Alanine scanning mutagenesis in the corresponding domains in VEGF revealed that charged amino acid residues in two exposed domains of VEGF are involved in binding to VEGFR-1 (Asp63, Glu64, and Glu67) and VEGFR-2 (Arg82, Lys84, and His86), respectively. Wang et al. (9) prepared a D63AE64AE67A mutant of VEGF_121_ (VEGF_DEE_) by changing Asp63, Glu64, and Glu67 to Ala63, Ala64, and Ala 67 so that the mutant could bind preferably to VEGFR-2 over VEGFR-1. VEGF_DEE_ was labeled with ^64^Cu via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) for imaging VEGFR-2 expression in an orthotopic 4T1 murine breast tumor model to develop ^64^Cu-labeled DOTA-VEGF_DEE_ (^64^Cu-DOTA-VEGF_DEE_) as a single-photon emission computed tomography (PET) imaging agent to study tumor angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE)+synthesis)]

^64^Cu labeling of VEGF_121_ and VEGF_DEE_ was performed through DOTA chelation. DOTA was activated by 1-ethyl-3-[3-(dimethylamino)-propyl] carbodiimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) at pH 5.5 for 30 min with a molar ratio of 10:5:4 (DOTA/EDC/SNHS) (9). The DOTA-VEGF_121_ conjugate was purified on a PD-10 column. The number of DOTA molecules per protein was ~2 for VEGF_121_ and VEGF_DEE_. For radiolabeling, 10 μg of VEGF_121_ or VEGF_DEE_ was added to 37 MBq (1 mCi) of ^64^CuCl_2_ diluted in 300 μl of 0.1 M sodium acetate buffer. The reaction mixture was incubated for 1 h at 40ºC. ^64^Cu-DOTA-VEGF_121_ and ^64^Cu-DOTA-VEGF_DEE_ were purified by PD-10 column chromatography. The ^64^Cu labeling time including final purification was ~80 min, and the radiolabeling yield was >85%. The specific activity was ~3.0 GBq/mg (81.1 mCi/mg). The radiochemical purity was >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE)+in+vitro)]

In vitro competition binding studies were performed in porcine aortic endothelial cells expressing cloned human VEGFR-1 and VEGFR-2 with the use of ^125^I-VEGF_165_ (9). VEGF_DEE_ exhibited ~19-fold lower binding to VEGFR-1 (IC_50_, 78.1 nM versus 4.2 nM) and ~3-fold lower binding to VEGFR-2 (IC_50_, 11.7 nM versus 2.9 nM) than VEGF_121_. The binding affinity of VEGF_DEE_ is ~6-fold higher to VEGFR-2 than that of VEGFR-1.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE)+rodentia)]

Wang et al. (9) performed biodistribution studies of ^64^Cu-DOTA-VEGF_121_ and ^64^Cu-VEGF_DEE_ in mice bearing 4T1 murine breast tumors expressing VEGFR-2. The organs with the highest accumulation of ^64^Cu-DOTA-VEGF_DEE_ were the liver (~20% injected dose per gram (% ID/g)), lung (~10% ID/g), and kidneys (~6% ID/g) at 4 h after injection. The tumor/muscle ratio was 6.0 for ^64^Cu-DOTA-VEGF_121_ and 5.6 for ^64^Cu-DOTA-VEGF_DEE_. The kidney was the only organ showing significant difference in radioactivity between the two tracers, with accumulation of ^64^Cu-DOTA-VEGF_DEE_ measured at <50% of ^64^Cu-DOTA-VEGF_121_ (P < 0.01) because rodent kidneys expressed high levels of VEGFR-1 based on immunofluorescence staining. PET imaging studies revealed that both ^64^Cu-DOTA-VEGF_121_ and ^64^Cu-DOTA-VEGF_DEE_ had rapid and prominent activity accumulation in the 4T1 tumor. The tumor uptake (% ID/g) of ^64^Cu-DOTA-VEGF_121_ was 3.6 ± 0.4 at 1 h, 4.6 ± 0.5 at 4 h, and 3.0 ± 0.2 at 20 h. ^64^Cu-DOTA-VEGF_DEE_ uptake in the tumor (% ID/g) was slightly higher at 4.6 ± 1.4 at 1 h, 5.0 ± 0.3 at 4 h, and 3.5 ± 0.5 at 20 h. Co-injection of 200 μg of VEGF_121_ reduced the tumor uptake of each tracer to <2.0% ID/g. The renal uptake of ^64^Cu-DOTA-VEGF_DEE_ was significantly lower than that of ^64^Cu-DOTA-VEGF_121_, whereas the uptake of each tracer in other organs was similar.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE)+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE)+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cu+VEGF(DEE)+human)]

No publication is currently available.

## NIH Support

R21 EB001785, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9. Wang, H., W. Cai, K. Chen, Z.B. Li, A. Kashefi, L. He, and X. Chen, A new PET tracer specific for vascular endothelial growth factor receptor 2. Eur J Nucl Med Mol Imaging, 2007.